# Sodium-2-[(3-butanoylamino-2,4,6-triiodo-phenyl)methyl]butanoate

Chemical name: | Sodium-2-[(3-butanoylamino-2,4,6-triiodo-phenyl)methyl]butanoate
Abbreviated name: | Tyropanoate sodium
Synonym: | Bilopaque®, WIN-8851-2, Lumopaque
Agent Category: | Compound
Target: | Gallbladder
Target Category: | Hepatic uptake and biliary excretion after oral absorption
Method of detection: | Planar X-ray, Computed Tomography (CT)
Source of signal/contrast: | Iodine
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%22tyropanoate%22[TIAB]%20NOT%20Medline[SB]%29%20OR%20%22tyropanoate%22[MeSH%20Terms]%20OR%20Bilopaque[Text%20Word])]

Sodium-2-[(3-butanoylamino-2,4,6-triiodo-phenyl)methyl]butanoate (tyropanoate sodium) is an oral X-ray cholecystographic agent used to aid the radiographic visualization of the gallbladder for detecting the presence of gallstones in cholelithiasis patients (1-4). Clinically, this technique is largely superseded by ultrasound, computed tomography (CT; without contrast), and nuclear medicine techniques and is used only for selected patients (5-7). Studies in 1999-2000 reported that it might be feasible to use this class of agents with helical CT cholangiography (8).

Radiographic imaging of the gallbladder depends on the opacification of the gallbladder with an oral cholecystographic agent. Solubilization in the intestinal lumen, absorption across the intestinal mucosa, transport in the blood, uptake and excretion by the liver and final concentration of the agent in the gallbladder allow X-ray imaging of the gallbladder and the biliary tree (9-12).

Cholecystographic agents are generally weak organic acids that contain a tri-iodinated benzene ring with iodine at positions 2, 4 and 6 (2, 7, 13-16). This class of compounds includes iocetamic acid, iopanoic acid, bunamiodyl sodium and ipodate. Their major chemical differences are the different substituents at positions 1 and 3 on the aromatic ring. The hydrophobic and hydrophilic properties of these substituents determine the aqueous and lipid solubility of the compound, and it must be sufficiently lipophilic to pass through the gastrointestinal mucosa. The absence of a substituent at position 5 allows the compound to bind to serum albumin and facilitates preferential hepatocyte uptake. The exact hepatic uptake mechanism is not entirely known. The agent is then metabolized by glucuronide conjugation in the same pathway as bilirubin (17-19). These glucuronide-conjugated compounds are readily excreted into the bile, follow the bile flow to fill up the gallbladder, and then are excreted by the biliary system in the feces.

Tyropanoate sodium was first synthesized in1962 as a modification of an earlier cholecystographic agent, iopanoic acid, in an effort to decrease its toxicity (1, 15, 20). Based on the fact that aromatic amino compounds are detoxified in vivo by acetylamino groups, tyropanoate sodium was developed and was different from iopanoic acid, chiefly in the butyrylation of the amine group. Whereas iopanoic acid is insoluble in water, tyropanoate sodium as a salt is soluble in water. The greater aqueous solubility of tyropanoate sodium and the lack of effect of bile acids on its hepatic excretion favor its oral absorption in the fasting state (21).

The commercial formulation of tyropanoate sodium contains approximately 57.4% iodine for producing the necessary X-ray attenuation and organ opacification (1, 2, 4). It is no longer marketed in the United States.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22[Substance%20Name]%20AND%20synthesis)]

Tyropanoate sodium was synthesized by butyrylation of the amine group of iopanoic acid (20). In this method, iopanoic acid was converted to tyropanoic acid by acidifying and heating with butyric anhydride at 70-80^o^C for 2 hours. A yield of 84% of Tyropanoic acid was obtained, and was then converted to tyropanoate sodium by the addition of methanolic sodium hydroxide.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28%22tyropanoate%22[TIAB]%20NOT%20Medline[SB]%29%20OR%20%22tyropanoate%22[MeSH%20Terms]%20OR%20Bilopaque[Text%20Word]%29%20AND%20%28%22in%20vitro%22[M)]

No specific in vitro cell uptake or metabolic study of tyropanoate sodium has been published. In a 1982 rat liver study of the deiodination mechanism of the tyrosyl and the phenolic ring of the thyroid hormones, tyropanoate sodium was shown capable of inhibiting competitively deiodination of thyroid hormones (22). In another study using patient serum, tyropanoate sodium was also found to competitively displace thyroid hormones from serum protein binding (23)

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28%22tyropanoate%22[TIAB]%20NOT%20Medline[SB]%29%20OR%20%22tyropanoate%22[MeSH%20Terms]%20OR%20Bilopaque[Text%20Word]%29%20AND%20%28%22rodentia%22[MeS)]

Acute toxicity studies in mice reported that the acute intravenous LD_50_ in mice for tyropanoate sodium was 720 mg/kg and the oral LD_50_ was 4.8-16.3 g/kg (20).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28%22tyropanoate%22[TIAB]%20NOT%20Medline[SB]%29%20OR%20%22tyropanoate%22[MeSH%20Terms]%20OR%20Bilopaque[Text%20Word]%29%20AND%20%28%28%28%22dogs%22[T)]

Preliminary imaging studies were performed in cats (20). The average cholecystographic index (ACI) using a visualization scoring scheme in cats for tyropanoate sodium (100 mg/kg) was reported to be 3.7 (13). In comparison, the ACI for iopanoic acid was 3.6.

With intravenous administration of tyropanoate sodium to dogs, the concentrations attained in the bile were approximately 60-400 times higher than the plasma concentrations (24). The urinary excretion of tyropanoate sodium was proportional to the plasma levels and accounted for about 30% of the total excretion. Both (+) and (-) enantiomers of tyropanoate glucuronide were identified in the plasma as tyropanoate sodium metabolites. Approximately 50% of the plasma tyropanoate sodium was glucuronide derivatives. In another study, the rate of biliary excretion of tyropanoate sodium was not significantly influenced by the rate of hepatic excretion of bile salts (11).

With oral administration of tyropanoate sodium to dogs, tyropanoate sodium reached a maximal iodine concentration of 11.5 ± 0.4 mg in the bile around 60 minutes after ingestion. This was higher than 2.2 ± 0.55 mg of iopanoic acid but similar to12.9 ± 1.4 mg of sodium ipodate (25). Excretion studies showed that tyropanoate sodium also caused a marked increase in bile flow (choleresis) which was not observed with iopanoate sodium (26). With the use of imaging techniques, data in dogs showed that opacification of the gallbladder might persist up to 4 days as measured by CT and up to 2.5 days by planar radiography (27). A study on the effect of diet and fasting showed no difference in mean gallbladder density measured by CT for a single dose given with a meal as compared with that in fasting. However, the density was significantly greater after a second dose when tyropanoate sodium was given in fasting (28).

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22[Substance%20Name]%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28%22tyropanoate%22[TIAB]%20NOT%20Medline[SB]%29%20OR%20%22tyropanoate%22[MeSH%20Terms]%20OR%20Bilopaque[Text%20Word]%29%20AND%20%28%28%22humans%22[TI)]

Human biochemical studies indicated that after oral ingestion of 4.5 g of tyropanoate sodium, tyropanoate sodium was rapidly absorbed from the intestinal tract and a peak serum iodine level of 330-460 mg/liter could be reached in 1-4 h (14, 15). Approximately 50% of tyropanoate sodium was excreted in the urine and 50% in the feces. In normal subjects, the gallbladder was optimally opacified 5-8 h after ingestion of tyropanoate sodium (29). The simultaneous administration of a meal with tyropanoate sodium appeared to impair gallbladder opacification (30). The effective absorbed dose for a typical cholecystography was reported to be about 2 mSv (200 mrem) (31). In comparison, the effective dose for a typical CT scan was estimated to be 8.8 mSv (880 mrem).

In patient studies with a 3 g dose of tyropanoate sodium, the time of peak visualization of the gallbladder with planar radiography after oral ingestion was 8-10 h (82-98% of 54 patients), whereas iopanoic acid could take 14-19 h (32, 33). In 13 patients with acute pancreatitis, the mean plasma level of tyropanoate sodium was 0.329 µmol/ml in 1-6 h compared with 0.061 µmol/ml for iopanoic acid (34).

In a retrospective study of 364 patient cases, the clinical performance of gallbladder visualization of tyropanoate sodium (4.5 g) appeared to be comparable to that of iopanoic acid (3 g) with fewer side effects (24.3% side effects for tyropanoate sodium and 48.7% side effects for iopanoic acid) (1). Another crossover comparison study of 50 patients who received both agents in 2 weeks reported improvement in gallbladder visualization for tyropanoate sodium (70% good visualization for tyropanoate sodium and 58% for iopanoic acid) with similarly fewer side effects (4). In 50 patients with acute alcoholic pancreatitis, 31% of the tyropanoate sodium (3 g) group achieved diagnostic single-dose cholecystograms, compared with only 11% of the iopanoic acid (3 g) group (34).

## References

1 Benisek G.J., Gunn J.A. (1962). A preliminary clinical evaluation of a new cholecystographic medium bilopaque. Am J Roentgenol Radium Ther Nucl Med.
2 Marshall T.R. (1976). Clinical comparison of locetamic acid, lopanoic acid and tyropanoate sodium. J Indiana State Med Assoc.
3 Pollack S. (1963). Clinical evaluation of a new cholecystographic agent: WIN 8851-2 (Bilopaque). Oklahoma State Medical Association.
4 Burhenne H.J. (1963). Bilopaque: A new cholecystographic medium. Radiology.
5 Fiske S.A., Stamper D.W. (1984). The use of calcium Oragrafin granules in repeat cholecystography, with supplemental ultrasonographic evaluation. J Am Osteopath Assoc.
6 Noguchi K., Suzuki H., Nakahata M., Kurosawa S., Nakagawa S. (1986). Prolonged treatment of hyperthyroidism with sodium tyropanoate, an oral cholecystographic agent: a re-evaluation of its clinical utility. Clin Endocrinol (Oxf).
7. Swanson, D.P., S.M. Simms, Cholecystographic and cholangiographic contrast media, in Pharmaceuticals in Medical Imaging, D.P. Swanson, H.M. Chilton and J.H. Thrall, Editor. 1990, MacMillan Publishing Co., Inc.: New York. p. 184-220.
8 Chopra S. (2000). K.N.C., K. Ramakrishna, H. Rhim and G.D. Dodd, Helical CT cholangiography wiht oral cholecystographic contrast material. Radiology.
9 Amberg J.R. Thompson W.M. Golberger L. Williamson S. Alexander R. Bates M. Factors in the intestinal absorption of oral cholecystopaques Invest Radiol 1980 15Suppl6 S136 41 7203915
10 Berk R.N., Loeb P.M. (1976). Pharmacology and physiology of the biliary radiographic contrast materials. Semin Roentgenol.
11 Berk R.N., Loeb P.M., Cobo-Frenkel A., Barnhart J.L. (1977). The biliary and urinary excretion of sodium tyropanoate and sodium ipodate in dogs: pharmacokinetics, influence of bile salts and choleretic effects with comparison to iopanoic acid. Invest Radiol.
12 Janes J.O., Dietschy J.M., Berk R.N., Loeb P.M., Barnhart J.L. (1979). Determinants of the rate of intestinal absorption of oral cholecystographic contrast agents in the dog jejunum. Gastroenterology.
13 Hoppe J.O., Archer S. (1953). Observations on a series of aryltriiodoalkanoic acid derivatives with particular reference to a new cholecystographic medium, Telepaque. American Journal of Radiology.
14 Davis J.J. (1964). Tyropanoate Sodium. A New Oral Cholecystographic Medium. Rocky Mt Med J.
15 Judkins M.P., Billimoria P.E., Dotter C.T. (1963). A comparative evaluation of a new oral cholecystographic agent bilopaque with orabilex. Am J Roentgenol Radium Ther Nucl Med.
16 Wishart D.L., Dotter C.T. (1973). Comparison of the opacifying characteristics and pharmacologic responses of iocetamic acid (Cholebrine), a new oral cholecystographic agent, with sodium tyropanoate (Bilopaque). Am J Roentgenol Radium Ther Nucl Med.
17. Loeb, P.M., R.N. Berk, Biliary contrast materials, in Radiology of the gallbladder and bile ducts, R.N. Berk, A.R. Clemett, Editor. 1977, W.B. Saunders Co.: Philadelphia. p. 71-100.
18 McChesney E.W. (1956). a.J.O.H., Observations on the absorption and excretion of the glucuronide of iopanoic acid in the cat. Arch Int Pharmacodyn Ther.
19 Muhletaler C.A., Gerlock A.J., Amberg J.R., Avant G.R. (1982). Radiographic appearance of the nonabsorbed (unconjugated) and conjugated sodium tyropanoate (bilopaque) in the bowel. Invest Radiol.
20 Hoppe J.O., Ackerman J.H., Larsen A.A., Moss J. (1970). Sodium tyropanoate, a new oral cholecystographic agent. Journal of Medicinal Chemistry.
21 Longstreth G.F., Slivka J. (1981). Tyropanoate cholecystography early in the course of acute pancreatitis. J Clin Gastroenterol.
22 Fekkes D., Hennemann G., Visser T.J. (1982). Evidence for a single enzyme in rat liver catalysing the deiodination of the tyrosyl and the phenolic ring of iodothyronines. Biochem J.
23 Felicetta J.V., Green W.L., Huber-Smith M.J. (1983). Effects of cholecystographic agents and sulfobromophthalein on binding of thyroid hormones to serum proteins. J Clin Endocrinol Metab.
24 Cooke W.J., Cooke L.M. (1983). Biliary and urinary excretion of tyropanoic acid and its Metabolites in the dog. Invest Radiol.
25 Menuck L., Amberg J.R., Bates M. (1977). Hepatic excretion of cholecystopaques introduced into the canine jejunum. Invest Radiol.
26 Nelson J.A., Straubus A.E., Amberg J.R. (1974). The choleretic action of sodium tyropanoate (bilopaque sodium) in the dog: preliminary observation. Invest Radiol.
27 Hunter T.B., Fon G.T., Berk R.N., Capp M.P. (1981). Concentration and excretion of contrast agents during oral cholecystography as measured by computed tomography in dogs. Gastrointest Radiol.
28 Fon G.T., Hunter T.B., Berk R.N., Capp M.P. (1980). The effect of diet and fasting on gallbladder opacification during oral cholecystography in dogs as measured by computed tomography. Radiology.
29 Muhletaler C.A., Gerlock A.J., Amberg J.R., Avant G.R. (1982). Radiographic appearance of the nonabsorbed (unconjugated) and conjugated sodium tyropanoate (Bilopaque) in the bowel. Invest Radiol.
30 Loeb P.M., Berk R.N., Janes J.O., Perkin L., Moore J. (1978). The effect of fasting on gallbladder opacification during oral cholecystography: a controlled study in normal volunteers. Radiology.
31 Ron E. (2003). Cancer risks from medical radiation. Health Phys.
32 Oliphant M., Whalen J.P., Evans J.A. (1974). Time of optimal gallbladder opacification with bilopaque (tyropanoate sodium). Radiology.
33 Han S.Y., Witten D.M. (1974). Clinical trial of bilopaque (tyropanoate sodium) oral cholecystography. Evaluation of time for the optimal and peak opacification of the gallbladder. Radiology.
34 Smith H.J., Corbett D.B., Loeb P.M., Peterson W.L. (1982). Oral cholecystography in the early phase of acute alcoholic pancreatitis. A prospective, randomized comparison of Telepaque and Bilopaque. Invest Radiol.